# [^99m^Tc](CO)_3_N-(pyridin-2-yl-methyl)-N[2-(4-sulfamoylphenyl)-ethyl]aminoethyl acetate

Chemical name: | [^99m^Tc](CO)_3_N-(pyridin-2-yl-methyl)-N[2-(4-sulfamoylphenyl)-ethyl]aminoethyl acetate
Abbreviated name: | [^99m^Tc]5
Synonym:
Agent Category: | Compound
Target: | Carbonic anhydrase IX
Target Category: | Enzyme
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure of [^99m^Tc]5 for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=anti-carbonic%20anhydrase%20antibodies&cmd=DetailsSearch)]

Hypoxic tumors are often resistant to radio- and chemotherapy, have a high metastatic potential, and predict a poor outcome for the cancer patient (1). Although several techniques (invasive and noninvasive) are available for the detection of hypoxia in tumors, these methods are not completely reliable because they yield variable diagnoses, have functional limitations, show incomplete penetration of tumors, or do not detect hypoxia in all tumor types (2, 3). A common feature of most solid cancerous tumor types is the presence of hypoxic conditions (2) and the overexpression of carbonic anhydrase IX (CA IX; exists in several isomeric forms), a transmembrane cell-surface metallo-enzyme that has been shown to acidify the pH of tumor cells to ~6.5 compared to pH ~7.4 for normal cells (4, 5). The induction of CA IX through the hypoxia-inducible factor-I transcription factor pathway and its role in tumorigenesis has been described in detail by Guler et al. (5). In view of its role in the development and progression of neoplastic tumors, oncologists and researchers are pursuing CA IX inhibitors for the detection or therapy of different cancer types. As a result, several small molecule inhibitors of CA are available, and among these compounds some sulfonamide derivatives have shown high selectivity for CA IX (6). It has also been shown that not only overexpression but also activation of the enzyme facilitates the accumulation of sulfonamides in a hypoxic tumor (7). Therefore, noninvasive imaging of CA IX would be an excellent technique to detect tumor hypoxia to develop a suitable treatment regimen for cancer patients. To achieve this, [^99m^Tc](CO)_3_N-(pyridin-2-yl-methyl)-N[2-(4-sulfamoylphenyl)-ethyl]aminoethyl acetate ([^99m^Tc]5) was synthesized and evaluated for the detection of CA IX (7). Biodistribution of the tracer was studied in mice bearing HT-29 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-38&Template=cellBiology) xenograft tumors because HT-29 cells express CA IX.

### Other Sources of Information

Hypoxia-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=Hypoxia+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Carbonic+anhydrase+IX+inhibitors) on CA IX inhibitors

Human CA IX in Entrez Gene (http://www.ncbi.nlm.nih.gov/gene/768) (Gene ID 768)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/169636419) of human CA IX

Human CA IX in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/nuccore?Db=omim&DbFrom=nuccore&Cmd=Link&LinkName=nuccore_omim&IdsFromResult=169636419) database

Hypoxia response in National Cancer Institute-Nature Pathways Interaction Database (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=100145&pathway_name=hypoxia-inducible%20factor%20in%20the%20cardivascular%20system&source=BioCarta%20Imported&what=graphic&jpg=on&ppage=1)

Crystal structure of the catalytic domain (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?Dopt=s&uid=76607) of the human CA IX

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99Tc-5%20synthesis&cmd=DetailsSearch)]

The synthesis of [^99m^Tc]5 has been described by Akurathi et al. (7). The radiochemical yield, purity, and specific activity of the tracer were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99Tc-5%20in%20vitro&cmd=DetailsSearch)]

To study the affinity of [^99m^Tc]5 for the I, II, IX, and XII isozymes of CA under in vitro conditions, a rhenium analog of the compound (Re-4) was used (7). Re-4 was reported to have K_i_ values (nM) of 3,440, 50, 58, and 45.1 for human CA isozymes I, II, IX, and XII, respectively. The selectivity of Re-4 (ratio of the K_i_ of CA IX to the K_i_ of XII) was determined to be 0.86.

Incubation of HT-29 cells in the presence of Re-4 under hypoxic conditions was reported to acidify the extracellular environment of the cells (from pH 7.4 to pH 6.9) (7). In addition, the hypoxic cells were shown to express approximately four-fold higher amounts of CA IX compared to the normal cells as determined with Western blot analysis. Using the same technique the investigators showed that a similar overexpression of the enzyme was observed in tumor cells analyzed under ex vivo conditions.

The distribution coefficient of [^99m^Tc]5 was determined with the shake flask and back extraction methods using a 1-octanol/phosphate buffer mixture (pH 7.4) as described by Akurathi et al. (7). The log D_octanol/buffer_ values for the tracer were reported to be 0.05 ± 0.00 and 0.06 ± 0.02, respectively, indicating that the radiochemical was moderately lipophilic.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99mTc-5%20rodentia&cmd=DetailsSearch)]

Akurathi et al. studied the biodistribution of [^99m^Tc]5 in anesthetized (2% isoflurane and 98% O_2_) NMRI-nu (nu/nu) mice bearing HT-29 cell xenograft tumors (7). The animals (n = 3 per time point) were euthanized at 0.5, 1, 2, and 4 h post-injection (p.i.), and the major organs were collected to determine the amount of accumulated radioactivity. The results were expressed as percent injected dose per gram tissue (% ID/g). The kidneys had the highest accumulation of the tracer with 36.0 ± 2.4% ID/g at 1 h p.i., which decreased to 17.8 ± 2.5% ID/g at 4 h p.i., followed by the liver (16.7 ± 2.8% ID/g and 3.1 ± 0.8% ID/g at 1 h and 4 h p.i., respectively) and the intestines (6.0 ± 0.3% ID/g and 17.6 ± 0.2% ID/g at 1 h and 4 h p.i., respectively). The tumors showed a negligible amount of radioactivity (0.1 ± 0.0% ID/g at 1 h p.i.), which was washed out by 4 h p.i. However, the tumor/blood ratio was reported to increase from 0.7 ± 0.2 at 1 h p.i. to 1.0 ± 0.1 at 4 h p.i.

Blocking studies were performed in mice (n = 3 animals per group) pretreated with unlabeled 4-(2-aminoethyl)benzenesulfonamide (a precursor of [^99m^Tc]5; 10 mg/kg body weight administered intraperitoneally) and injected with the radiochemical 1 h later (7). Control animals were not treated with the unlabeled precursor. The animals were euthanized 1 h after the [^99m^Tc]5 injection, and the highest radioactivity was detected in the liver (35.68 ± 1.91% ID/g compared to 43.10 ± 2.86% ID/g for the control mice), followed by the intestines (35.54 ± 4.0% ID/g compared to 36.52 ± 3.40% ID/g for the control mice) and kidneys (17.67 ± 1.86% ID/g compared to 17.35 ± 3.73% ID/g for the control mice). The amount of radioactivity accumulated in the tumors was not reported.

Possible reasons for almost no accumulation of [^99m^Tc]5 in the tumors have been described elsewhere (7). On the basis of the results obtained from the different studies, the investigators concluded that [^99m^Tc]5 was not a suitable tracer for the detection of tumors expressing CA IX (7).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99Tc-5%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99Tc-5%20Non-Human%20Primates&cmd=DetailsSearch)]

No publications are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=99Tc-5%20Human%20Studies&cmd=DetailsSearch)]

No publications are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Michalski, M.H. and X. Chen, Molecular imaging in cancer treatment. Eur J Nucl Med Mol Imaging, 2010
2 Carlin S., Khan N., Ku T., Longo V.A., Larson S.M., Smith-Jones P.M. (2010). Molecular targeting of carbonic anhydrase IX in mice with hypoxic HT29 colorectal tumor xenografts. PLoS One.
3 Mees G., Dierckx R., Vangestel C., Van de Wiele C. (2009). Molecular imaging of hypoxia with radiolabelled agents. Eur J Nucl Med Mol Imaging.
4 De Simone G., Supuran C.T. (2010). Carbonic anhydrase IX: Biochemical and crystallographic characterization of a novel antitumor target. Biochim Biophys Acta.
5 Guler O.O., De Simone G., Supuran C.T. (2010). Drug design studies of the novel antitumor targets carbonic anhydrase IX and XII. Curr Med Chem.
6 Winum J.Y., Scozzafava A., Montero J.L., Supuran C.T. (2009). Inhibition of carbonic anhydrase IX: a new strategy against cancer. Anticancer Agents Med Chem.
7 Akurathi V., Dubois L., Lieuwes N.G., Chitneni S.K., Cleynhens B.J., Vullo D., Supuran C.T., Verbruggen A.M., Lambin P., Bormans G.M. (2010). Synthesis and biological evaluation of a 99mTc-labelled sulfonamide conjugate for in vivo visualization of carbonic anhydrase IX expression in tumor hypoxia. Nucl Med Biol.